# 2-tert-Butyl-4-chloro-5-[4-(4-[^18^F]fluoro-butyl)-benzyloxy]-2H-pyridazin-3-one

Chemical name: | 2-tert-Butyl-4-chloro-5-[4-(4-[^18^F]fluoro-butyl)-benzyloxy]-2H-pyridazin-3-one
Abbreviated name: | [^18^F]RP1004
Synonym:
Agent category: | Compound
Target: | Mitochondrial complex 1 (MC1)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1004)]

Lipophilic cations are capable of passing through biological membranes by passive diffusion into the cytoplasm and mitochondria of cells in response to large negative plasma and mitochondrial membrane potentials. ^99m^Tc-2-Methoxyisobutylisonitrile (^99m^Tc-MIBI) and ^99m^Tc-tetrofosmin are delocalized lipophilic cations, which are rapidly taken up into cells driven by metabolic demand and membrane potential (1-4). They are used as myocardial-perfusion single-photon emission computed tomography agents and as tumor-imaging agents. However, the high accumulation of Tc tracers in the lung and liver may interfere with the detection of flow abnormalities in the myocardium. More recently, positron emission tomography (PET) imaging has emerged as an alternative approach to evaluating myocardial blood flow by use of positron-emitting radionuclides (e.g., ^82^RbCl, ^13^NH_3_, and H_2_^15^O). However, the majority of these radiotracers exhibited short physical half-lives (<10 min). Lipophilic cations such as [^11^C]triphenylmethylphosphonium ([^11^C]TPMP) (5) and 4-[^18^F]fluorobenzyl-triphenylphosphonium ([^18^F]FBnTP) have been investigated as PET agents for myocardial and tumor imaging (6).

Mitochondrial complex I (MC1) of the mammalian electron transfer chain is composed of at least 43 protein subunits, of which 7 are encoded by mitochondrial DNA (7). MC1 catalyzes the transfer of electrons from NADH to ubiquinone and translocates protons from the mitochondrial matrix to the intermembrane space to generate ATP and thus the energy supply of the cell. MC1 may also play direct roles in the mitochondrial permeability transition and in cell death pathways. Myocardium has a high mitochondrial content because of high energy usage. 2-tert-Butyl-4-chloro-5-[4-(4-fluoro-butyl)-benzyloxy]-2H-pyridazin-3-one (RP1004) is found to be a potent MC1 inhibitor with a hydrophobic heterocyclic pyridazinone (8). 2-tert-Butyl-4-chloro-5-[4-(4-[^18^F]fluoro-butyl)-benzyloxy]-2H-pyridazin-3-one ([^18^F]RP1004) has been synthesized to study its use as a PET agent for imaging myocardium.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Mitochondrial%20complex+AND+micad%5Bbook%5D)
- Gene information in NCBI (MC1 receptors (http://www.ncbi.nlm.nih.gov/gene/291))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/252010)
- Clinical trials (MC1 (http://www.clinicaltrials.gov/ct2/results?term=Mitochondrial+complex+1+))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1004+synthesis)]

[^18^F]RP1004 was prepared as described by Yu et al. (8). [^18^F]Fluoride/Kryptofix 2.2.2/K_2_CO_3_ and the tosylate precursor were heated in acetonitrile for 30 min at 90°C, followed by high-performance liquid chromatography purification. Total synthesis time was 90 min. Radiochemical purity was >90% with specific activities of 27.8–55.5 GBq/µmol (0.75–1.5 Ci/µmol) at the end of synthesis. [^18^F]RP1004 exhibited a calculated log P value of 4.84.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1004%20and%20in%20vitro)]

Yu et al. (8) reported that RP1004 inhibited NADH oxidation by bovine heart submitochondrial particles with a 50% inhibition concentration (IC_50_) value of 16.7 nM. The IC_50_ value of known MC1 inhibitor rotenone was 18.2 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1004%20and%20rodentia)]

Yu et al. (8) performed ex vivo biodistribution studies of [^18^F]RP1004 in rats (n = 9). [^18^F]RP1004 accumulated mainly in the heart with 2.40 ± 0.21% injected dose/g (ID/g) and 2.67± 0.27% ID/g at 15 min and 60 min after injection, respectively. Retention of [^18^F]RP1004 in the heart was good with no washout. The heart/blood, heart/lung, heart/liver, and heart/femur ratios were 33.3, 12.1, 1.5, and 3.4 at 60 min after injection, respectively. The uptake in the femur was 0.78% ID/g at 60 min, indicating some defluorination of [^18^F]RP1004. For comparison, heart accumulation of ^99m^Tc-sestamibi was 2.0% ID/g at 60 min with a heart/lung ratio of 5.9 at 60 min after injection. PET imaging showed that [^18^F]RP1004 accumulated mainly in the heart and liver with low accumulation in the lung. Good myocardial images were observed at 25–35 min after injection with little interference from the lung and liver at 55–60 min. No blocking experiment was performed. The first pass extraction efficiency was not addressed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F%20RP1004+and+(dog+or+pig+or+sheep+or+rabbit))]

Yu et al. (8) performed PET imaging studies of [^18^F]RP1004 in rabbits (n = 6). [^18^F]RP1004 accumulated mainly in the myocardium within minutes after injection, with some interference from the lung and liver at 5–15 min after injection. Retention of [^18^F]RP1004 in the heart was good with little washout, whereas the retention was much lower in the liver. Accumulation of [^18^F]RP1004 in the heart was clearly visualized at 65 min after injection with no interference from the lung and liver accumulation of [^18^F]RP1004.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1004%20and%20%28primate%20not%20human%29)]

Yu et al. (8) performed PET imaging studies of [^18^F]RP1004 in two rhesus monkeys. [^18^F]RP1004 accumulated mainly in the myocardium within 5–15 min of injection. Retention of [^18^F]RP1004 in the heart was good with no washout, whereas the retention was much lower in the liver with >58% loss of radioactivity. Accumulation of [^18^F]RP1004 in the heart was clearly visualized at 60 min after injection with no interference from the liver accumulation of [^18^F]RP1004.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1004%20and%20human)]

No publication is currently available.

## References

1 Chernoff D.M., Strichartz G.R., Piwnica-Worms D. (1993). Membrane potential determination in large unilamellar vesicles with hexakis(2-methoxyisobutylisonitrile)technetium(I). Biochim Biophys Acta.
2 Chiu M.L., Kronauge J.F., Piwnica-Worms D. (1990). Effect of mitochondrial and plasma membrane potentials on accumulation of hexakis (2-methoxyisobutylisonitrile) technetium(I) in cultured mouse fibroblasts. J Nucl Med.
3 Molteni S.N., Seregni E., Botti C., Martinetti A., Ferrari L., Crippa F., Bombardieri E. (1999). The breast cancer cell line MCF7 as a model of 99mTc-SestaMIBI, 99mTc-tetrofosmin and 99mTc-Medronate incorporation. Anticancer Res.
4 Younes A., Songadele J.A., Maublant J., Platts E., Pickett R., Veyre A. (1995). Mechanism of uptake of technetium-tetrofosmin. II: Uptake into isolated adult rat heart mitochondria. J Nucl Cardiol.
5 Krause B.J., Szabo Z., Becker L.C., Dannals R.F., Scheffel U., Seki C., Ravert H.T., Dipaola A.F., Wagner H.N. (1994). Myocardial perfusion with [11C]methyl triphenyl phosphonium: measurements of the extraction fraction and myocardial uptake. J Nucl Biol Med.
6 Madar I., Ravert H.T., Du Y., Hilton J., Volokh L., Dannals R.F., Frost J.J., Hare J.M. (2006). Characterization of Uptake of the New PET Imaging Compound 18F-Fluorobenzyl Triphenyl Phosphonium in Dog Myocardium. J Nucl Med.
7 Lenaz G., Fato R., Genova M.L., Bergamini C., Bianchi C., Biondi A. (2006). Mitochondrial Complex I: structural and functional aspects. Biochim Biophys Acta.
8 Yu M., Guaraldi M., Kagan M., Mistry M., McDonald J., Bozek J., Yalamanchili P., Hayes M., Azure M., Purohit A., Radeke H., Casebier D.S., Robinson S.P. (2009). Assessment of 18F-labeled mitochondrial complex I inhibitors as PET myocardial perfusion imaging agents in rats, rabbits, and primates. Eur J Nucl Med Mol Imaging.